# 3-{4-[2-[Benzoxazol-2-yl-methylamino]ethoxy]phenyl}-2-(2-[^18^F]fluoroethoxy)propionic acid

Chemical name: | 3-{4-[2-[-Benzoxazol-2-yl-methylamino]ethoxy]phenyl}-2-(2-[^18^F]fluoroethoxy)propionic acid
Abbreviated name: | Compound [^18^F]22
Synonym:
Agent Category: | SB 213 068
Target: | Peroxisome proliferator–activated receptor γ
Target Category: | Receptor binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PPARgamma)]

Peroxisome proliferator–activated receptors (PPARs), once considered orphan receptors, are now believed to be the primary modulators of glucose and lipid metabolism in animals. PPARs are also believed to regulate the storage and catabolism of dietary fat (1). There are three subtypes of the receptors, designated as PPAR-α, PPAR-β/δ, and PPAR-γ (2). Among these, PPAR-γ is the most extensively investigated and has been cloned from a variety of species including fish, amphibians, rodents, and mammals (2). PPAR-γ has been shown to be an important transcription factor receptor that regulates adipocyte differentiation (3), represses the ob gene that regulates leptin expression (4), and modulates obesity and inflammation in mice (5). There is evidence that activation of PPAR-γ can have an anti-carcinogenic effect on colon cancer (6), and that PPAR-γ can alter the malignant phenotype of some human colon carcinoma cell lines (7, 8). PPAR-γ levels were shown to be elevated in breast cancer cell lines and during metastases in animal tumor models for breast cancer (9). Although PPAR-γ ligands induced tumor differentiation in animal models, not all cell lines that were positive for PPAR-γ respond to the ligands. With these observations the investigators suggest receptor phosphorylation may be necessary for responsiveness because the phosphorylated receptor had a low ligand affinity (10), which led to a reduced responsiveness of S112 cells that probably had a previously phosphorylated receptor (11). Kim et al (12). suggest that the nonphosphorylated form of PPAR-γ may be a novel target for tumor therapy and that radiotracers could be used to identify tumors retaining the ability to bind the ligands. They suggest that functional imaging of the tumors may help identify, and allow direction of therapy for, patients who are most likely to benefit. This would reduce time lost in providing therapies to individuals who are unlikely to respond to treatment, as such patients could be provided alternative therapies.

In an effort to develop a radiotracer compound that could be used to study tissue distribution of PPAR-γ and provide a high contrast between target and non-target tissue, Kim et al. selected a very potent synthetic ligand belonging to the 3-phenylpropionic acid (SB 213 068) class of compounds, a [^18^F]fluorine-substituted analog, 3-{4-[2-[-(benzoxazol-2-yl-methylamino])ethoxy]phenyl}-2-(2-[^18^F]fluoroethoxy)propionic acid (12), also designated as compound [^18^F]22. The tissue distribution of compound [^18^F]22 was studied in two animal models (rats and SCID mice) by the investigators.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PPAR%20ligand%20synthesis)]

The synthesis of compound [^18^F]22 was described by Kim et al. (12). For this, methyl 3-[-{4-[2-[-(benzoxazol-2-yl-methylamino])ethoxy]phenyl]-}-2-(2-[^18^F]fluoroethoxy)propanoate was used as the base compound. It was prepared by incubation of tetrabutylammonium [^18^F]fluoride (n-BuN4[^18^F]F) with 3-[-{4-[2-[benzoxazol-2-yl-methylamino])ethoxy]phenyl}-2-(2-fluoroethoxy)acrylic acid at 80^o^C in an oil bath for 30 min. The substituted ^18^F methyl ester was purified by semipreparative high-performance liquid chromatography (HPLC) on a silica column. The labeled ester was dissolved in methanol and 10% NaOH solution, and then heated at 80^o^C for 15 min. The solution was then acidified with 1N HCl and extracted with hexane, passed through MgSO_4_, and purified by semipreparative HPLC. Fractions containing compound [^18^F]22 were combined, counted, and concentrated under reduced pressure. The typical radiochemical yield was 20–30%, decay corrected from (n-BuN4[^18^F]F), and the entire synthesis process took 2.5–3.5 h.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F-PPAR%20gamma%20ligand)]

The binding affinity of compound [^18^F]22 was determined by competitive binding as described earlier (13, 14) using receptor preparations that consisted of the ligand-binding domains expressed in Escherichia coli. The K_i_ and K_d_ of compound [^18^F]22 for PPAR-γ were determined to be 7 nM and ~5 nM, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F-PPAR%20gamma%20ligand%20rodentia)]

The distribution of compound [^18^F]22 was studied in two animal models, adult rats and SCID mice bearing human breast tumor MCF-7 xenografts (12). On the basis of mRNA expression, the highest PPAR-γ levels were expected in the brown and white adipose tissue, and significant levels were also expected in the spleen and mucosa of the duodenum (12). The MCF-7 cells are positive for the estrogen receptor, require estradiol for growth, and exhibit a high level of PPAR-γ. Therefore, a significant level of the receptors would be expected to be present in the xenografts (12).

Female Sprague-Dawley rats (200–225 g) were administered a low (5 µCi) or high (30 µCi) dose of compound [^18^F]22 through the tail vein. A group of animals also received a blocking dose as a combination of unlabeled and labeled compound [^18^F]22. Animals were sacrificed 1 h after administration of the low or high dose, with or without the block, whereas animals sacrificed after 3 h that received only the low dose, with or without the block, were sacrificed after 3 h. Blood and tissue from these animals were collected, weighed, and counted for radioactivity.

Tissue distribution of compound [^18^F]22 was expected to be similar to the distribution of PPAR-γ given above and it was expected to be displaced by the unlabelled compound. However, the investigators observed that compound [^18^F]22 did not have a tissue selective uptake, and high levels were observed only in the liver and kidney. Uptake in the white and brown adipose tissue was not significantly different from that of other tissue such as the heart and muscle. The investigators were unable to evaluate the uptake in duodenal mucosa because a high level of the radiotracer was present in the intestinal contents, probably as a result of compound [^18^F]22 metabolite excretion through the hepatobiliary system.

Female SCID mice were implanted with MCF-7 cells by subcutaneous injections in the left and right flanks, and the tumors were allowed to grow for 4 weeks in presence of estradiol; each animal had a timed-release estradiol pellet (1.7 mg/60 days) inserted at the side of the neck. The tumor-bearing animals were treated with cold or labeled compound [^18^F]22 as detailed above for the rats. Tissues from these animals were collected as described for the rats, and the gall bladder and tumors were also harvested. With the SCID mice, uptake was observed mainly in the liver, kidney, and the lungs. A high uptake in the gall bladder was also observed, which indicated that the tracer was excreted through the hepatobiliary system, as observed with the rats. Uptake in the other tissues of the SCID mice was also similar to that observed in the rats. In addition, the investigators observed that uptake in the tumors was not different, selective, or blocked, similar to observations in the other tissues.

With data obtained from this study (12), Kim et al. concluded that uptake of compound [^18^F]22 in the normal tissue or tumors was not selective as expected. The investigators recommend the development of compounds with better tissue selectivity that can be used to perform uptake and imaging studies. For this purpose, Kim et al. discuss the possible use of a tyrosine-benzophenone class of compounds that have a higher affinity and invivo potency against PPAR-γ. However, in their opinion, it would be a challenge to develop imaging agents for PPAR-γ (12).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F-PPAR%20gamma%20non-primate%20mammals)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F-PPAR%20gamma%20Non-Human%20Primates)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F-PPAR%20gamma%20Human%20Studies)]

No publications are currently available.

## References

1 Nolte RT, Wisely GB, Westin S, Cobb JE, Lambert MH, Kurokawa R, Rosenfeld MG, Willson TM, Glass CK, Milburn MV. (1998). Ligand binding and co-activator assembly of the peroxisome proliferator-activated receptor-gamma. Nature.
2 Willson TM, Brown PJ, Sternbach DD, Henke BR. (2000). The PPARs: from orphan receptors to drug discovery. J Med Chem.
3 Tontonoz P, Hu E, Spiegelman BM. (1994). Stimulation of adipogenesis in fibroblasts by PPAR gamma 2, a lipid-activated transcription factor. Cell.
4 De Vos P, Lefebvre AM, Miller SG, Guerre-Millo M, Wong K, Saladin R, Hamann LG, Staels B, Briggs MR, Auwerx J. (1996). Thiazolidinediones repress ob gene expression in rodents via activation of peroxisome proliferator-activated receptor gamma. J Clin Invest.
5 Stienstra R, Mandard S, Patsouris D, Maass C, Kersten S, Muller M. (2007). and , PPAR{alpha} protects against obesity-induced hepatic inflammation. Endocrinology.
6 Bull AW. (2003). The role of peroxisome proliferator-activated receptor gamma in colon cancer and inflammatory bowel disease. Arch Pathol Lab Med.
7 Kato M, Kusumi T, Tsuchida S, Tanaka M, Sasaki M, Kudo H. (2004). Induction of differentiation and peroxisome proliferator-activated receptor gamma expression in colon cancer cell lines by troglitazone. J Cancer Res Clin Oncol.
8 Sarraf P, Mueller E, Jones D, King FJ, DeAngelo DJ, Partridge JB, Holden SA, Chen LB, Singer S, Fletcher C, Spiegelman BM. (1998). Differentiation and reversal of malignant changes in colon cancer through PPARgamma. Nat Med.
9 Mueller E, Sarraf P, Tontonoz P, Evans RM, Martin KJ, Zhang M, Fletcher C, Singer S, Spiegelman BM. (1998). Terminal differentiation of human breast cancer through PPAR gamma. Mol Cell.
10 Shao D, Rangwala SM, Bailey ST, Krakow SL, Reginato MJ, Lazar MA. (1998). Interdomain communication regulating ligand binding by PPAR-gamma. Nature.
11 Hu E, Kim JB, Sarraf P, Spiegelman BM. (1996). Inhibition of adipogenesis through MAP kinase-mediated phosphorylation of PPARgamma. Science.
12 Kim SH, Jonson SD, Welch MJ, Katzenellenbogen JA. (2001). Fluorine-substituted ligands for the peroxisome proliferator-activated receptor gamma (PPARgamma): potential imaging agents for metastatic tumors. Bioconjug Chem.
13 Nichols JS, Parks DJ, Consler TG, Blanchard SG. (1998). Development of a scintillation proximity assay for peroxisome proliferator-activated receptor gamma ligand binding domain. Anal Biochem.
14 Xu HE, Lambert MH, Montana VG, Parks DJ, Blanchard SG, Brown PJ, Sternbach DD, Lehmann JM, Wisely GB, Willson TM, Kliewer SA, Milburn MV. (1999). Molecular recognition of fatty acids by peroxisome proliferator-activated receptors. Mol Cell.